# Annexin A5-Gd-micelles-Cy5.5

Chemical name: | Annexin A5-Gd-micelles-Cy5.5
Abbreviated name: | AnxA5-micelles
Synonym:
Agent category: | Protein
Target: | Phosphatidylserine
Target category: | Phospholipid
Method of detection: | Multimodality imaging: magnetic resonance imaging (MRI), optical (near-infrared (NIR) fluorescence)
Source of signal\contrast: | Iron oxide, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20and%20micelles)]

Optical fluorescence imaging is increasingly being used to obtain images of biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in small animals.

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (3). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal (3). On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

A multimodal nanoparticle probe that consists of a contrast agent and a NIR fluorochrome may provide consistent imaging information. CLIO nanoparticles can be internalized by cells of the reticuloendothelial system and have long circulating times within an animal body. The blood half-life of CLIO is ~10 h in mice (4). The accumulation of nanoparticles in cells causes a reduction in signal intensity with T2-weighted (T2*W) spin-echo pulse sequences. NIR fluorochromes (e.g., Cy5.5) provide an improved optical (NIR) signal from tissue. CLIO-Cy5.5 has been developed as a multimodal probe for imaging.

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, atherosclerosis, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (5). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) (5) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V (or annexin A5) binding in necrosis because of disruption of the plasma membrane. Annexin V, a 36-kDa protein, binds to PS with high affinity (K_d_ = 7 nM). Annexin V has been radiolabeled with ^123^I, ^124^I, and ^99m^Tc for single-photon emission computed tomography (SPECT) imaging (6-8). Annexin V was successfully labeled with ^18^F (^18^F-labeled annexin V (4-[^18^F]FBA)) (9, 10) and is currently being developed as a positron emission tomography agent for imaging apoptosis as well as necrosis (11). Cy5.5-Annexin V has been evaluated as an optical probe in small animals. Annexin V-CLIO-Cy5.5 (AnxCLIO-Cy5.5 (http://www.ncbi.nlm.nih.gov/books/NBK23475/)) is a multimodal agent that consists of CLIO nanoparticles labeled with annexin V and Cy5.5 (12). van Tilborg et al. (13) incorporated annexin A5 into di-stearoyl-polyethylene glycol-phosphatidylethanolamine 2000 (DSPE-PEG2000) micelles labeled with Gd-DTPA and Cy5.5 (Annexin A5-Gd-micelles-Cy5.5 (AnxA5-micelles)) for multimodality imaging of atherosclerotic plaques.

### Related Resource Links:

- Chapters in MICAD (Annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Annexin%20V+AND+micad%5Bbook%5D))
- Gene information in NCBI (Annexin V (http://www.ncbi.nlm.nih.gov/gene/308))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Annexin V (http://www.ncbi.nlm.nih.gov/omim/131230))
- Clinical trials (Annexin V (http://www.clinicaltrials.gov/ct2/results?term=Annexin+V+))
- Drug information in FDA (Annexin V (http://google2.fda.gov/search?q=annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20synthesis)]

DSPE-PEG2000, Gd-DTPA-bisstearylamide, and maleimide-PEG2000-DSPE in a molar ratio of 40:50:10 were mixed in chloroform (13). Cy5.5-PEG2000-DSPE (1 mol %) was added to the mixture, and the solution was dried by rotary evaporation for 3 min at 40°C. The lipid film was subsequently hydrated with 4 ml HEPES-buffered saline to form micelles. Annexin A5-cys was conjugated to the maleimide-PEG2000-DSPE-micelles by sulfhydryl-maleimide bonding. AnxA5-Micelles were purified with dialysis. Control micelles without annexin A5 were prepared similarly. The hydrodynamic diameters of AnxA5-micelles and control micelles were determined to be 22.3 ± 0.2 nm and 19.5 ± 0.7 nm, respectively. There were two annexin A5 molecules, one Cy5.5 molecule, and 40 Gd molecules per AnxA5-micelle. AnxA5-micelles and control micelles exhibited r1 relaxivity values of 12.4 mM^-1^s^-1^ and 13.4 mM^-1^s^-1^ in HEPES-buffered saline at 1.5 T and 37°C, whereas Gd-DTPA exhibited an r1 relaxivity value of 3.3 mM^-1^s^-1^ under the same conditions.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20in%20vitro)]

van Tilborg et al. (13) performed cell-binding assays with AnxA5-micelles and control micelles in apoptotic human Jurkat T cells with the use of confocal laser scanning microscopy. The apoptotic cells incubated with AnxA5-micelles showed a clear cell-associated fluorescence signal, whereas negligible fluorescence signal was obtained with control micelles.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20rodentia)]

van Tilborg et al. (13) used a 9.4-T MRI scanner to perform in vivo T1-weighted MRI in apolipoprotein E–deficient (ApoE^-/-^) mice, which exhibit severe atherosclerosis in the abdominal area. AnxA5-Micelles (n = 3, 2.5 µmol lipid, 50 µmol Gd/kg, 53 nmol annexin A5) and control micelles (n = 3, 2.5 µmol lipid, 50 µmol Gd/kg) were injected in ApoE^-/-^ mice. Pre-injection scans showed extensive atherosclerotic lesions in the aorta in ApoE^-/-^ mice but not in wild-type mice (n = 2). Contrast enhancement was observed within the width of the aortic wall in ApoE^-/-^ mice at 24 h after injection of AnxA5-micelles and persisted for up to 7 days. No contrast change was observed in the aorta of wild-type mice at 24 h after injection of control micelles. Furthermore, atherosclerotic lesions in ApoE^-/-^ mice injected with control micelles showed less signal enhancement at 24 h after injection. Ex vivo biodistribution of AnxA5-micelles and control micelles in ApoE^-/-^ mice was assessed in the liver, spleen, kidney, and lung by measurement of Gd content at 24 h after injection. The kidney and lung showed <5 µg/g Gd concentration, and results were similar with both micelles. On the other hand, Gd content was 50 µg/g in the liver and 42 µg/g in the spleen with AnxA5-micelles, whereas Gd content was 25 µg/g in the liver and 12 µg/g in the spleen with control micelles. Mean MRI signal in the aortic wall was calculated to be increased by 10.7 ± 1.7% and 6.7 ± 3.4% with AnxA5-micelles and control-micelles, respectively. The total NIR photon measurement in the entire aorta was enhanced by 257.1 ± 9.1% and 113.1 ± 4.4% with AnxA5-micelles and control micelles, respectively. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20micelles%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
4 Wunderbaldinger P., Josephson L., Bremer C., Moore A., Weissleder R. (2002). Detection of lymph node metastases by contrast-enhanced MRI in an experimental model. Magn Reson Med.
5 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
6 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
7 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
8 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
9 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
10 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
11 Medarova Z., Pham W., Farrar C., Petkova V., Moore A. (2007). In vivo imaging of siRNA delivery and silencing in tumors. Nat Med.
12 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
13 van Tilborg G.A., Mulder W.J., Deckers N., Storm G., Reutelingsperger C.P., Strijkers G.J., Nicolay K. (2006). Annexin A5-functionalized bimodal lipid-based contrast agents for the detection of apoptosis. Bioconjug Chem.